# 2-(6-Chloro-2-(4-(3-[^18^F]fluoropropoxy)phenyl)imidazo[1,2-a]pyridin-3-yl)-N,N-diethylacetamide

Chemical name: | 2-(6-Chloro-2-(4-(3-[^18^F]fluoropropoxy)phenyl)imidazo[1,2-a]pyridin-3-yl)-N,N-diethylacetamide
Abbreviated name: | [^18^F]PBR111
Synonym:
Agent category: | Compound
Target: | Peripheral-type benzodiazepine receptor (PBR), also known as translocator protein (TSPO)
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR111%5BAll%20Fields%5D)]

Benzodiazepines are potent psychoactive drugs used for their sedative and anxiolytic properties (1, 2). There are two types of benzodiazepine receptors, which have been designated as central benzodiazepine receptors (CBR) and peripheral benzodiazepine receptors (PBR). The CBR is found exclusively in the central nervous system on the membranes of neurons and is coupled to the γ-aminobutyric acid receptor/chloride channel (3). In contrast, the PBR is a mitochondrial protein found in brain and peripheral tissues (adrenal gland, heart, lung, kidney, and testis) (4). The brain has lower levels of PBR than do peripheral tissues. Both glial cells and macrophages contain high levels of PBR (5-7). Increased PBR expression after brain injury or neuroinflammation is associated with microglial activation, such as occurs with the neuronal damage that accompanies several neurodegenerative diseases, including Alzheimer’s disease, Wernicke’s encephalopathy, multiple sclerosis, and epilepsy.

PBRs have been studied in vivo with positron emission tomography (PET) using 1-(2-chlorophenyl)-N-[^11^C]methyl-N-(1-methylpropyl)-3-isoquinoline carboxamide ([^11^C]PK11195), an isoquinoline carboxamide with specific PBR antagonistic activity. [^11^C]PK11195 has been developed as a PET agent for non-invasive studies of microglia and macrophage activation in the brain, lung, and heart. However, accumulation of this tracer in the brain is limited. N-(2,5-Dimethoxybenzyl)-N-(5-fluoro-2-phenoxyphenyl)acetamide (DAA1106) was found to be a selective agonist for studying PBRs in the central nervous system (8, 9). DAA1106 was reported to have a higher affinity for PBRs in mitochondrial fractions of rat and monkey brains than PK11195 (8, 9). Therefore, both tracers are able to cross the normal cell membrane to reach the mitochondrial receptor sites. N-(5-Fluoro-2-phenoxyphenyl)-N-(2-[^18^F]fluoroethyl-5-methoxybenzyl)acetamide ([^18^F]FEDAA1106) and [^11^C]DAA1106 have been developed as potential PET ligands with highly selective and specific binding to PBR (10, 11). 2-(6-Chloro-2-(4-(3-[^18^F]fluoropropoxy)phenyl)imidazo[1,2-a]pyridin-3-yl)-N,N-diethylacetamide ([^18^F]PBR111) has been evaluated for imaging PBR (12).

### Related Resource Links:

- Chapters in MICAD (PBR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=PBR%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (PBR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=706%5Buid%5D))
- Articles in OMIM (PBR (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=109610))
- Clinical trials (PBR (http://www.clinicaltrials.gov/ct2/results?term=pk11195+OR+PBR))
- Drug information in FDA (PBR (http://google2.fda.gov/search?q=Peripheral-type+benzodiazepine+receptor+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=5&y=5))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR111%20and%20synthesis)]

Fookes et al. (12) reported the synthesis of [^18^F]PBR111 by nucleophilic fluorination of the p-toluenesulfonyl precursor with [^18^F]KF/Kryptofix 2.2.2./K_2_CO_3_ at 100°C for 5 min and purified with high-performance liquid chromatography with a radiochemical purity of >95%. The specific activity was 110–150 GBq/μmol (2.97–4.05 Ci/μmol) at the end of synthesis with 56–75% radiochemical yield. The total preparation time was ~60 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR111%20and%20in%20vitro)]

In vitro [^3^H]PK11195 PBR-binding studies using PBR111 in rat kidney and brain membranes showed inhibition constant (K_i_) values of 3.7 ± 0.4 nM and 800 ± 120 nM for PBR and CBR, respectively (12).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR111%20and%20rodentia)]

Fookes et al. (12) reported biodistribution studies of [^18^F]PBR111 in rats that showed high accumulation of radioactivity in the adrenal gland (11.8% injected dose (ID)/g), followed by the heart (8.3% ID/g), lung (7.7% ID/g), spleen (6.0% ID/g), and kidney (5% ID/g) at 30 min after injection of [^18^F]PBR111. The level of radioactivity was low in the brain (0.2% ID/g), blood (0.3% ID/g), and the olfactory bulbs (0.6% ID/g). In the femur, the accumulation of radioactivity was 0.4% ID/g at 15 min and 2.2% ID/g at 4 h. Pretreatment with 1 mg/kg PK11195 or 1 mg/kg PBR111 decreased the accumulation in the heart, kidney, and spleen by >75% but had no effect in the adrenal gland, blood, and brain at 60 min after injection. There was a decrease of ~50% in the olfactory bulbs in the brain. Pretreatment with flumazenil (a CBR ligand) exhibited little effect on the [^18^F]PBR111 radioactivity level in the heart, kidney, spleen, and olfactory bulbs. The fraction of unchanged [^18^F]PBR111 at 15 min after injection was 10% in the blood plasma, 80% in the brain cortex, and 95% in the olfactory bulbs.

Van Camp et al. (13) performed PET imaging in rats with acute neuroinflammation. PET imaging showed an increased accumulation of [^18^F]PBR111 in the lesion as compared to the contralateral side as early as 6 min after injection. Administration of an excess of PK11195 and PBR111 (20 min after [^18^F]PBR111 injection) induced a rapid and complete displacement of [^18^F]PBR111 binding from the lesion. Modeling of the PET data using the simplified reference tissue model showed significant (P < 0.001) increase in binding potential (BP) of [^18^F]PBR111 (2.5 ± 0.7) in comparison to [^11^C]PK11195 (1.1 ± 0.2). Only intact [^18^F]PBR111 was detected in the brain up to 60 min after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR111%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR111%20and%20%28primate%20not%20human%29)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR111%20and%20human)]

No publications are currently available.

## NIH Support

Intramural research program

## References

1 Mohler H., Okada T. (1977). Benzodiazepine receptor: demonstration in the central nervous system. Science.
2 Hunkeler W., Mohler H., Pieri L., Polc P., Bonetti E.P., Cumin R., Schaffner R., Haefely W. (1981). Selective antagonists of benzodiazepines. Nature.
3 Olsen R.W., Tobin A.J. (1990). Molecular biology of GABAA receptors. Faseb J.
4 Anholt R.R., Pedersen P.L., De Souza E.B., Snyder S.H. (1986). The peripheral-type benzodiazepine receptor. Localization to the mitochondrial outer membrane. J Biol Chem.
5 Jones H.A., Valind S.O., Clark I.C., Bolden G.E., Krausz T., Schofield J.B., Boobis A.R., Haslett C. (2002). Kinetics of lung macrophages monitored in vivo following particulate challenge in rabbits. Toxicol Appl Pharmacol.
6 Kuhlmann A.C., Guilarte T.R. (2000). Cellular and subcellular localization of peripheral benzodiazepine receptors after trimethyltin neurotoxicity. J Neurochem.
7 Zavala F., Lenfant M. (1987). Benzodiazepines and PK 11195 exert immunomodulating activities by binding on a specific receptor on macrophages. Ann N Y Acad Sci.
8 Okuyama S., Chaki S., Yoshikawa R., Ogawa S., Suzuki Y., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Neuropharmacological profile of peripheral benzodiazepine receptor agonists, DAA1097 and DAA1106. Life Sci.
9 Chaki S., Funakoshi T., Yoshikawa R., Okuyama S., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Binding characteristics of [3H]DAA1106, a novel and selective ligand for peripheral benzodiazepine receptors. Eur J Pharmacol.
10 Fujimura Y., Ikoma Y., Yasuno F., Suhara T., Ota M., Matsumoto R., Nozaki S., Takano A., Kosaka J., Zhang M.R., Nakao R., Suzuki K., Kato N., Ito H. (2006). Quantitative analyses of 18F-FEDAA1106 binding to peripheral benzodiazepine receptors in living human brain. J Nucl Med.
11 Maeda J., Suhara T., Zhang M.R., Okauchi T., Yasuno F., Ikoma Y., Inaji M., Nagai Y., Takano A., Obayashi S., Suzuki K. (2004). Novel peripheral benzodiazepine receptor ligand [11C]DAA1106 for PET: an imaging tool for glial cells in the brain. Synapse.
12 Fookes C.J., Pham T.Q., Mattner F., Greguric I., Loc'h C., Liu X., Berghofer P., Shepherd R., Gregoire M.C., Katsifis A. (2008). Synthesis and biological evaluation of substituted [18F]imidazo[1,2-a]pyridines and [18F]pyrazolo[1,5-a]pyrimidines for the study of the peripheral benzodiazepine receptor using positron emission tomography. J Med Chem.
13 Van Camp, N., R. Boisgard, B. Kuhnast, B. Theze, T. Viel, M.C. Gregoire, F. Chauveau, H. Boutin, A. Katsifis, F. Dolle, and B. Tavitian, In vivo imaging of neuroinflammation: a comparative study between [(18)F]PBR111, [ (11)C]CLINME and [ (11)C]PK11195 in an acute rodent model. Eur J Nucl Med Mol Imaging, 2010